# ^11^C-Labeled isoniazid

Chemical name: | ^11^C-Labeled isoniazid | [image]
Abbreviated name: | [^11^C]INH | [image]
Synonym: | ^11^C-Labeled isonicotinylhydrazine | [image]
Agent Category: | Compounds | [image]
Target: | Synthesis of mycolic acid | [image]
Target Category: | Enzymes (bacteria) | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^11^C | [image]
Activation: | No | [image]
Studies: | - In vitro; - Non-human primates | Structure of [^11^C]INH by Liu et al (1). Click on the PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance?term=isoniazid) for additional information about INH.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=drug+development+and+PET+imaging+and+review)]

Isoniazid, also known as isonicotinylhydrazine (INH), is a first-line drug used in the prevention and treatment of tuberculosis (TB) (1, 2). INH is a prodrug that is activated by the catalase-peroxidase enzyme KatG of the mycobacteria. The activation process leads to the formation of the isonicotinic acyl-NADH complex. Subsequent binding of the complex with the enoyl-acyl carrier protein reductase InhA results in the inhibition of mycolic acid synthesis, which is essential for the wall of mycobacteria (3). INH is bactericidal to rapidly dividing mycobacteria but is bacteriostatic to slow-growing mycobacteria. INH labeled with ^11^C ([^11^C]INH) has been generated by Liu et al. for in vivo and real-time analysis of the INH pharmacokinetics (PK) and biodistribution with positron emission tomography (PET) (1). The half-life of ^11^C is 20.4 min, allowing for a ~60 min window to observe the PK.

The PK and biodistribution of a novel drug are traditionally determined with blood and tissue sampling and/or autoradiography. Despite high workload and huge investment in drug development, only 8% of the drugs entering clinical trials today reach the market, as estimated by the U.S. Food and Drug Administration (http://www.fda.gov/ScienceResearch/SpecialTopics/CriticalPathInitiative/CriticalPathOpportunitiesReports/ucm077262.htm). One main reason for this attrition is insufficient exploration of the in vivo drug–target interaction (1). Traditional methods are inadequate to answer questions such as whether a drug reaches the target, how the drug interacts with its targets, and how the drug modifies the diseases. Because of the high resolution and sensitivity of newly developed imaging techniques, investigators have become increasingly interested in addressing these issues (4, 5). In the case of PET imaging, most small molecules can now be efficiently labeled with ^11^C or with ^18^F at >37 GBq/µmol (1 Ci/μmol), and they can be detected with PET in the nanomolar to picomolar concentration range (6-8). Consequently, a sufficient signal for imaging can be obtained even though the total amount of a radiotracer administered systemically is extremely low (known as microdosing, typically <1 μg for humans). Microdosing is particularly valuable for evaluating tissue exposure in the early phase of drug development when the full-range toxicology is not yet available (9, 10). Increasing evidence has demonstrated the efficiency of PET imaging in obtaining quantitative information on drug PK and distribution in various tissues including brain; confirming drug binding with targets and elucidating the relationship between occupancy and target expression/function in vivo; assessing drug passage across the blood–brain barrier (BBB) and ensuring sufficient exposure to brain for central nervous system drugs; and dissecting the modifying effects of drugs on diseases (4, 6, 7).

The current treatment regime for drug-sensitive TB involves the use of rifampicin (RIF), INH, pyrazinamide (PZA), and ethambutol or streptomycin for two months, followed by four months of continued dosing with INH and RIF (11, 12). This regime is primarily based on PK studies in serum and on efficacy of treatment. The efficacy of each drug for different types of TB such as brain TB and the drug distribution in each compartment of an organ are not well understood. To provide direct insights into these drugs, Liu et al. labeled INH, RIF, and PZA with ^11^C and used PET to investigate their PK and biodistribution in baboons (1). Liu et al. found that the organ distribution and BBB penetration of each drug differed greatly. The ability of [^11^C]INH to penetrate the BBB was lower than that of PZA but higher than that of RIF (PZA > INH > RIF). The INH concentrations in the lungs and brain were ten times higher than the INH minimum inhibitory concentration (MIC) value against TB, supporting the use of INH for treating TB infections in the lungs and brain. This chapter summarizes the data obtained by Liu et al. regarding [^11^C]INH. The data obtained with regard to [^11^C]RIF and [^11^C]PZA are described in the MICAD chapters on [^11^C]RIF and [^11^C]PZA, respectively.

### Related Resource Links:

- Challenge and Opportunity on the Critical Path to New Medical Products, FDA (http://www.fda.gov/ScienceResearch/SpecialTopics/CriticalPathInitiative/default.htm)
- Isoniazid compounds in PubChem Substance (http://www.ncbi.nlm.nih.gov/sites/entrez?db=pcsubstance&term=Isoniazid)
- Clinical trials for diagnosis and treatment of tuberculosis in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=tuberculosis)
- MICAD chapters on [^11^C]RIF and [^11^C]PZA (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20205479)]

Liu et al. synthesized [^11^C]INH in three steps, starting with [^11^C]HCN. The first step involved treatment of iodopyridine with [^11^C]HCN and catalysis with tetrakis(triphenylphosphine)palladium to form [^11^C]cyanopyridine. This step gave 90% radiochemical yield. Subsequent hydrazine hydrolysis of the cyanide was accomplished in two steps, which involved a nucleophilic attack by hydrazine and subsequent hydrolysis of the imine by water.

The final product was generated with an average 45%–50% decay-corrected yield (calculated from [^11^C]HCN) with a total synthesis time of 50 min. Isonicotinamide was the only major byproduct, with <15% of the total yield being isonicotinamide. The radiolabeled product was >99% radiochemically pure with a specific activity of 5.18–5.92 GBq/µmol (140–165 mCi/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20205479)]

Liu et al. determined the plasma protein binding (% of free fraction in plasma) of [^11^C]INH after incubation with baboon plasma for 10 min at room temperature. The plasma protein binding was 27.32%, which is similar to literature values reported elsewhere (1). The lipophilicity of [^11^C]INH was not measured.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

No references are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20205479)]

Liu et al. used PET imaging to study the biodistribution of [^11^C]INH in healthy baboons (n = 4) (1). The INH concentrations in the brain and other organs were estimated on the basis of the weight of the baboon, a standard daily dose (5 mg/kg for a human adult), and the assumption that the positron signal derives primarily from the intact drug. Studies showed that the penetrating ability of [^11^C]INH through the BBB was weaker than that of PZA but better than that of RIF. The INH concentration in the brain tissue was higher than in the cerebrospinal fluid. The concentration in the whole brain was 0.00299% injected dose per cubic centimeter (ID/cc) (2.54 μg/ml) at 30 min, 0.00248% ID/cc (2.11 μg/ml) at 60 min, and 0.00206% ID/cc (1.75 μg/ml) at 90 min after injection, which was ten times higher than its MIC against TB, suggesting that INH is a suitable drug for the treatment of brain TB infection as previously recommended.

The detailed data about the [^11^C]INF distribution in other organs were presented in table 3 in the paper published by Liu et al (1). In general, [^11^C]INH and/or its metabolites rapidly penetrated the heart, lungs, liver, and kidneys. In most organs, the INH concentration exceeded that observed in plasma over the 90-min period. The calculated concentration was more than ten times higher than its MIC, supporting the use of INH for treating TB infections. However, Liu et al. noticed in the literature differences between the INH concentrations in organs among different species, which were explained by the interspecies variation and radionuclide difference (1).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Liu L., Xu Y., Shea C., Fowler J.S., Hooker J.M., Tonge P.J. (2010). Radiosynthesis and bioimaging of the tuberculosis chemotherapeutics isoniazid, rifampicin and pyrazinamide in baboons. J Med Chem.
2 Hall R.G., Leff R.D., Gumbo T. (2009). Treatment of active pulmonary tuberculosis in adults: current standards and recent advances. Insights from the Society of Infectious Diseases Pharmacists. Pharmacotherapy.
3 Lu X.Y., You Q.D., Chen Y.D. (2010). Recent progress in the identification and development of InhA direct inhibitors of Mycobacterium tuberculosis. Mini Rev Med Chem.
4 Fox G.B., Chin C.L., Luo F., Day M., Cox B.F. (2009). Translational neuroimaging of the CNS: novel pathways to drug development. Mol Interv.
5 Komoda F., Suzuki A., Yanagisawa K., Inoue T. (2009). Bibliometric study of radiation application on microdose useful for new drug development. Ann Nucl Med.
6 Hammond L.A., Denis L., Salman U., Jerabek P., Thomas C.R., Kuhn J.G. (2003). Positron emission tomography (PET): expanding the horizons of oncology drug development. Invest New Drugs.
7 Lancelot, S. and L. Zimmer, Small-animal positron emission tomography as a tool for neuropharmacology. Trends Pharmacol Sci, 2010
8 Lee C.M., Farde L. (2006). Using positron emission tomography to facilitate CNS drug development. Trends Pharmacol Sci.
9 Bauer M., Wagner C.C., Langer O. (2008). Microdosing studies in humans: the role of positron emission tomography. Drugs R D.
10 Wagner C.C., Muller M., Lappin G., Langer O. (2008). Positron emission tomography for use in microdosing studies. Curr Opin Drug Discov Devel.
11 Tomioka H. (2006). Current status of some antituberculosis drugs and the development of new antituberculous agents with special reference to their in vitro and in vivo antimicrobial activities. Curr Pharm Des.
12 Aristoff P.A., Garcia G.A., Kirchhoff P.D., Hollis Showalter H.D. (2010). Rifamycins--obstacles and opportunities. Tuberculosis (Edinb).